# Cy5.5-Containing matrix metalloproteinase (MMP) activatable peptide conjugated to glycol chitosan (GC)–coated gold nanoparticles (AuNPs)

Chemical name: | Cy5.5-Containing matrix metalloproteinase (MMP) activatable peptide conjugated to glycol chitosan (GC)–coated gold nanoparticles (AuNPs)
Abbreviated name: | MMP-GC-AuNPs
Synonym:
Agent Category: | Nanoparticles (gold)
Target: | Matrix metalloproteinase (MMP)
Target Category: | Enzyme
Method of detection: | Multimodal imaging (optical imaging (OI); computed tomography (CT))
Source of signal / contrast: | Cy5.5/Au
Activation: | Yes
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://www.ncbi.nlm.nih.gov/pcsubstance).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=gold%20nanoparticles%20and%20molecular%20imaging&cmd=DetailsSearch)]

The use of gold nanoparticles (AuNPs) for molecular imaging has attracted much attention because these particles are easy to fabricate in different shapes, have a quenching effect, and can be used for computed tomography (CT) (1). Because bare AuNPs are unstable (due to aggregation) and are non-targeted, these particles have to be to be coated with biocompatible materials to improve their stability and application under in vivo conditions. In addition, NPs that are targeted to specific cellular biomarkers are useful for the detection and treatment of diseases such as cancers (for details, see Jiao et al. (2) and Lim et al. (3)). However, the AuNP surface coatings (e.g., thiolated polyethylene glycol) may influence the biological behavior of these particles and prevent their uptake by cells. This can result in reduced clearance of the NPs through the reticuloendothelial system, prolonged blood circulation times, and increased accumulation in tumors (4). Therefore, investigators are devoting much effort to develop AuNPs that are easy to synthesize, physiologically stable, and can be used to detect (e.g., by noninvasive imaging) and treat cancerous tumors (1). In an effort to produce AuNPs that would meet this criteria, the particles were coated with glycol chitosan (GC) and conjugated to a Cy5.5-containing matrix metalloproteinase (MMP) activatable peptide (Cy5.5-Gly-Pro-Leu-Gly-Val-Arg-Gly-Lys-black hole quencher-3 (BHQ-3) dye (http://www.biosearchtech.com/support/applications/dyes-from-biosearch-technologies/black-hole-quencher%C2%AE-dyes)-Gly-Gly; the MMP cleavable site is in italics) to produce MMP-GC-AuNPs for use as a multimodal computed tomography (CT)/near-infrared fluorescence (NIRF) imaging probe (1). The MMP-GC-AuNPs were then evaluated with CT and NIRF optical imaging techniques for the visualization of HT-29 cell (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-38&Template=cellBiology) xenograft tumors (these cells express the MMP-2) in nude mice.

### Related Resource Links

Multimodal agents in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=Multimodal+AND+micad%5Bbook%5D+AND+table%5Btype%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

MMP-related chapters in MICAD (http://www.ncbi.nlm.nih.gov/books/?term=MMP+AND+micad%5Bbook%5D&view=chapter&p%24a=&p%24l=PBooksLayout&p%24st=books)

Clinical trials (http://clinicaltrials.gov/ct2/results?term=matrix+metalloproteinase) related to matrix metalloproteinase

MMP in Online Mendelian Inheritance in Man Database (OMIM (http://omim.org/entry/120360))

MMP in Kyoto Encyclopedia of Genes and Genomes (http://www.genome.jp/dbget-bin/www_bfind_sub?mode=bfind&max_hit=1000&dbkey=kegg&keywords=Matrix+metalloproteinase)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MMP-GC-AuNPs%20synthesis&cmd=DetailsSearch)]

The synthesis, formulation, and storage of the MMP-GC-AuNPs is described by Sun et al. (1). Based on the standard absorption curve of Cy5.5 at 675 nm, 572 molecules of the MMP peptide probe were reported to be conjugated to each GC-AuNP. Transmission electron microscopy showed that the MMP-GC-AuNPs had a spherical shape and a diameter of 20 nm. The GC layer on the AuNPs was uniform with a thickness of 10 nm, and the hydrodynamic diameter of the NPs in an aqueous solution was 99.4 ± 16.8 nm as determined with dynamic light scattering. The ζ potential of the MMP-GC-AuNPs was 34.48 ± 1.00 mV.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MMP-GC-AuNPs%20in%20vitro&cmd=DetailsSearch)]

The MMP-GC-AuNPs were reported to be stable in distilled water and phosphate-buffered saline from pH 3 to pH 11 for at least 80 days, and they maintained their diameter during this period (1). A cell proliferation assay with HeLa cells (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=CCL-2&Template=cellBiology) exposed to MMP-GC-AuNPs for 24 h showed that the NPs were non-toxic to the cells even at a concentration of 1 mg/mL in the growth medium (1).

MicroCt imaging of the MMP-GC-AuNPs showed that the particles had superior X-ray absorption properties compared with eXIA™160 (http://www.skyscan.be/products/contrast_agent.htm), an iodine-based contrast agent used for CT (1).

The investigators reported that 90% of the NIRF signal of MMP-GC-AuNPs was quenched by the fluorescence resonance energy transfer from the BHQ-3 component of the MMP activatable peptide (1). The NIRF of the gold NPs was recovered only in presence of MMP-2, and the NIRF intensity was shown to increase with the concentration of the enzyme.

Exposure of SCC-7 cells (express and secrete the MMP into the growth medium) to MMP-GC-AuNPs for 1 h showed that a strong fluorescence signal was generated with as little as 10^4^ cells (1). This indicated that the MMP-GC-AuNPs had a high sensitivity to the activity of the MMP enzymes.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MMP-GC-AuNPs%20rodentia&cmd=DetailsSearch)]

Nude mice bearing HT-29 cell tumors (number of animals not reported) were injected with the MMP-GC-AuNP probe (200 μL, 300 mg/kg body weight (BW)) through the tail vein, and the rodents were anesthetized to acquire whole-body CT images after different time periods (1). In the CT images, the tumor was clearly distinguishable from the surrounding tissues at 2 h postinjection (p.i.), and at 24 h p.i. the Hounsfield units (http://www.fpnotebook.com/Rad/CT/HnsfldUnt.htm) value for the lesions was 254, which was approximately five-fold higher than the normal surrounding tissues (Hounsfield units value = ~40). The lesions were not visible when eXIA™160 was used as the contrast agent for the CT imaging of the tumors (1). The investigators attributed this to the lack of tumor specificity and fast clearance of the eXIA™160 contrast agent from the body.

For NIRF imaging, the tumor-bearing animals (number of mice not reported) were injected with 200 μL (5 mg/kg BW) of the MMP-GC-AuNPs as before, and NIRF optical images were acquired from the animals at various time points (1). At 1 h p.i., an increased NIRF signal was apparent only in the tumor compared with the normal surrounding tissues, and the lesions were clearly visible from 4 h p.i. to 48 h p.i. In a blocking study, the animals were injected with the probe 30 min after intratumoral injection of a MMP inhibitor (the inhibitor was not specified), and no NIRF signal was generated in the tumor. At 4 h p.i., the mice (with or without the MMP inhibitor treatment) were euthanized, and organs of interest were removed from the animals. NIRF images of the organs showed that the tumor was clearly distinguishable from rest of the organs. Among all the organs, a low NIRF signal was observed only in the liver. Dark field microscopy of the various tissues confirmed the presence of MMP-GC-AuNPs in the tumors, including those treated with the MMP inhibitor. In addition, generation of the NIRF signal and the presence of the MMP enzymes in the tumor tissues was confirmed with optical fluorescence microscopy and immunostaining (for MMP), respectively (1).

On the basis of these results, the investigators concluded that the MMP-GC-AuNPs accumulated specifically in the tumor tissues and could be used as a dual CT/NIRF probe for the detection of cancerous tumors in rodents (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MMP-GC-AuNPs%20Other%20Non-Primate%20Mammals&cmd=DetailsSearch)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MMP-GC-AuNPs%20Non-Human%20Primates&cmd=DetailsSearch)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=MMP-GC-AuNPs%20Human%20Studies&cmd=DetailsSearch)]

No publication is currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Sun I.C., Eun D.K., Koo H., Ko C.Y., Kim H.S., Yi D.K., Choi K., Kwon I.C., Kim K., Ahn C.H. (2011). Tumor-targeting gold particles for dual computed tomography/optical cancer imaging. Angew Chem Int Ed Engl.
2 Jiao P.F., Zhou H.Y., Chen L.X., Yan B. (2011). Cancer-targeting multifunctionalized gold nanoparticles in imaging and therapy. Curr Med Chem.
3 Lim Z.Z., Li J.E., Ng C.T., Yung L.Y., Bay B.H. (2011). Gold nanoparticles in cancer therapy. Acta Pharmacol Sin.
4 Arnida M.M. (2011). Janat-Amsbury, A. Ray, C.M. Peterson, and H. Ghandehari, Geometry and surface characteristics of gold nanoparticles influence their biodistribution and uptake by macrophages. Eur J Pharm Biopharm.